# ^111^In-CHX-A”-diethylenepentaacetic acid-Affibody Z_HER2:2395_-Cys

Chemical name: | ^111^In-CHX-A”-diethylenepentaacetic acid-Affibody Z_HER2:2395_-Cys
Abbreviated name: | ^111^In-CHX-A’’-DTPA-Z_2395_-C
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | Epidermal growth factor (EGF) HER2 receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395)]

Epidermal growth factor (EGF) is a cytokine of 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_D_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_D_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A cysteine molecule was introduced at the C-terminus of Affibody molecules to form Affibody Z_HER2:2395_-Cys (Z_2395_-C) for site-specific coupling with the chelator [[2-(bis-carboxymethyl-amino)-cyclohexyl]-(2-bis-carboxymethyl-amino)-3-{4-[7-(2,5-dioxo-2,5-dihydro-pyrrol-1-ul)-heptanoylamino]-phenyl}-propyl)-amino]-acetic acid (maleimido-CHX-A’’-DPTA) for ^111^In labeling. ^111^In-CHX-A’’-DTPA-Affibody Z_HER2:2395_-Cys (^111^In-CHX-A’’-DTPA-Z_2395_-C) has been evaluated in nude mice bearing human colon adenocarcinoma tumors (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20synthesis)]

Affibody Z_2395_-C was reduced with dithiothreitol in 0.02 M ascorbic acid for 18 h at 37°C (18). The reduced Z_2395_-C was incubated with maleimido-CHX-A”-DTPA in 1:2 molar ratio in ammonium acetate buffer (pH 5.5) for 18 h at 37°C. The coupling efficiency was >99% as determined by LC-MS analysis. There was ~1 chelator per antibody. MMA-CHX-A”-DTPA-Z_2395_-C was isolated with column chromatography. MMA-CHX-A”-DTPA-Z_2395_-C (20 ug) was mixed with 18 MBq (0.49 mCi) ^111^InCl_3_ and incubated for 60 min. The labeling efficiency of ^111^In incorporation was >99%. Specific activity of the preparation was 6.3 GBq/µmol (170 mCi/µmol). ^111^In-CHX-A”-DTPA-Z_2395_-C was found to be stable after incubation for 4 h in the presence of excess ethylenediamine tetraacetic acid.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20in%20vitro)]

Tolmachev et al. (18) performed binding experiments with Z_2395_-C with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_D_ value of His_6_-Z_HER2:342_-C was calculated to be 29 pM. The K_D_ value of CHX-A”-DTPA-Z_2395_-C was 56 pM. Hence, the binding affinity of CHX-A”-DTPA-Z_2395_-C was only slightly lower than the parent Affibody molecule Z_HER2:342_, which had the K_D_ value of 22 pM (19). In vitro binding specificity tests showed that binding of ^111^In-CHX-A”-DTPA-Z_2395_-C to SKOV-3 cells expressing HER2 was receptor-mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^111^In-CHX-A’’-DTPA-Z_2395_-C. The cell-bound radioactivity remained at 81% of the initially bound activity for up to 24 h when the cells were incubated with ^99m^Tc-Z_2395_-C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20rodentia)]

Tolmachev et al. (18) performed ex vivo biodistribution studies of 0.1 MBq (2.7 μCi) ^111^In-CHX-A’’-DTPA-Z_2395_-C in nude mice bearing LS174T xenograft tumors. ^99m^Tc-Z_2395_-C (0.14 nmol) was injected intravenously into each mouse. The initial tracer accumulation in the LS174T tumors was 17% injected dose per gram (ID/g) at 1 h., 17% ID/g at 4 h and 8% ID/g at 24 h after injection. The radioactivity level in tumors was higher than in other organs and tissues (the lung, liver, spleen, and intestines) except in the kidneys (150–220% ID/g) at these time points. Blood levels were ~0.22% ID/g at 4 h. The biodistribution was characterized by rapid clearance of radioactivity from blood. Tumor/blood ratios were 12, 86, and 157 at 1, 4, and 24 h after injection, respectively. Preadministration of Z_HER2:342_ (520 µg (73 nmol)) decreased tumor accumulation by >90% (P = 0.001) at 4 h after injection.

Single-photon emission computed tomography analysis was performed in nude mice bearing the LS174T tumors after injection of 2.7 MBq (73 μCi) ^111^In-CHX-A’’-DTPA-Z_2395_-C. The tumor was clearly visualized at 1 h along with the kidneys. The tumor/muscle ratios were 20 and 37 at 1 h and 4 h, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%202395%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Tolmachev V., Xu H., Wallberg H., Ahlgren S., Hjertman M., Sjoberg A., Sandstrom M., Abrahmsen L., Brechbiel M.W., Orlova A. (2008). Evaluation of a maleimido derivative of CHX-A'' DTPA for site-specific labeling of affibody molecules. Bioconjug Chem.
19 Ahlgren S., Wallberg H., Tran T.A., Widstrom C., Hjertman M., Abrahmsen L., Berndorff D., Dinkelborg L.M., Cyr J.E., Feldwisch J., Orlova A., Tolmachev V. (2009). Targeting of HER2-expressing tumors with a site-specifically 99mTc-labeled recombinant affibody molecule, ZHER2:2395, with C-terminally engineered cysteine. J Nucl Med.